# (R,S)-anti-1-Amino-2-[^18^F]fluorocyclopentyl-1-carboxylic acid

Chemical name: | (R,S)-anti-1-Amino-2-[^18^F]fluorocyclopentyl-1-carboxylic acid
Abbreviated name: | anti-2-[^18^F]FACPC, [^18^F]FACPC
Synonym:
Agent category: | Compound
Target: | L-type and A-type amino acid transporters
Target category: | Amino acid transporters
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facpc%5BAll%20Fields%5D)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissue (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, L-[^11^C]methionine, and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid ([^11^C]ACPC), and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in imaging in oncology (4-6). The natural amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system and retained in tumor cells because of their higher than normal metabolic pathways, including incorporation into proteins (4). L-[^11^C]Methionine (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.MET11C) and [^18^F]fluorotyrosine (http://www.ncbi.nlm.nih.gov/books/bv.fcgi?rid=micad.chapter.FMT18F) have been widely used in the detection of tumors, but are not approved by the FDA. On the other hand, the non-natural amino acids are not metabolized but are taken up through both the L-type transporter and the energy-dependent A-type transporter (7). Therefore, they can accumulate intracellularly in high concentrations. In this chapter, (R,S)-anti-1-Amino-2-[^18^F]fluorocyclopentyl-1-carboxylic acid (anti-2-[^18^F]FACPC), a fluorinated analog of [^11^C]ACPC, was shown to have a high tumor/brain ratio in mice (8). However, anti-2-[^18^F]FACPC exhibited unfavorable imaging characteristics for detection of pelvic recurrent prostate carcinoma in five patients because of high blood level at 5 min and high urinary bladder level at 20 min (9).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D)
- Gene information in NCBI (L-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (Amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters))
- Drug information in FDA (Amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACPC+and+synthesis)]

Nucleophilic fluorination of syn-3-(N-(tert-butoxycarbonyl)amino)-4-cyclopentane-1,2,3-oxathiazolidine-4-carboxylic acid tert-butyl ester 2,2-dioxide with K[^18^F]F/Kryptofix2.2.2 was performed for 10 min at 110°C (8). Subsequent acid hydrolysis for 10 min at 110°C and purification provided a radiosynthesis yield of 39 ± 8% (decay-corrected, n = 4) of anti-2-[^18^F]FACPC at the end of synthesis. A radiochemical purity of 99% was obtained. The total synthesis time was 60 min from the end of bombardment. The specific activity of anti-2-[^18^F]FACPC was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACPC+and+in+vitro)]

anti-2-[^18^F]FACPC showed a fast uptake into rat 9L gliosarcoma tumor cells in culture with 6.33 ± 0.47% injected dose (10)/5 × 10^5^ cells (n = 3) at 30 min of incubation (8). The uptake was reduced by 71%, 38%, and 65% by the presence of 10 mM 2-aminobicyclo[2.2.1]heptane-2-carboxylic acid (L-type transporter inhibitor), N-methyl-α-aminoisobutyric acid (A-type transporter inhibitor), and a mixture of alanine, cysteine, and serine (ACS), respectively. The data suggest that anti-2-[^18^F]FACPC is a predominantly L-type transporter substrate with some affinity to the A-type transporter.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACPC+and+rodentia)]

Ex vivo biodistribution studies of anti-2-[^18^F]FACPC were performed in rats (n = 5/group) implanted intracerebrally with 9L gliosarcoma (8). Accumulation of anti-2-[^18^F]FACPC in the tumors was 0.57, 1.68, 1.24, and 0.98% ID/g at 15, 30, 60, and 120 min after injection, respectively. The accumulation in the contralateral brain tissue was ~0.11% ID/g at these time points. The tissue with the highest accumulation at 30 min after injection was the kidney (3.44% ID/g), followed by the pancreas (2.91% ID/g), lung (1.13% ID/g), and liver (0.63% ID/g). The accumulation in other tissues (heart, spleen, muscle, bone) was low (<0.5% ID/g). The tumor/brain and tumor/muscle ratios were 10–13 and ~5 at 30 min and 120 min, respectively. [^18^F]FDG exhibited a tumor/brain ratio of 0.84 at 60 min in the same tumor model (11). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACPC+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=FACPC+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=facpc%5BAll%20Fields%5D%20AND%20human)]

Savir-Baruch et al. (9) studied five patients with elevated PSA after curative therapy for prostate carcinoma underwent 60-min dynamic PET/CT of the pelvis after injection of 193-340 MBq (5.2-9.3 mCi) anti-2-[^18^F]FACPC. Average standard uptake value (SUV) of malignant lesions was 4.1 ± 1.3 and 2.6 ± 1.0 at 5 and 20 min, respectively. The lesion/blood ratios were 1.4 ± 0.5 at 5 min, whereas lesions/urinary bladder ratio was 0.3 ± 0.8 at 20 min. It was concluded that anti-2-[^18^F]FACPC exhibited unfavorable imaging characteristics for detection of pelvic recurrent prostate carcinoma because of high blood level at 5 min and high urinary bladder level at 20 min. On the other hand, anti-[^18^F]FACBC exhibited the lesion/blood and lesion/urinary bladder ratios of 3.0 ± 0.9 at 5 min and 2.3 ± 1.4 at 20 min, respectively.

## NIH Support

R01 CA129356

## References

1 Coleman R.E., Hoffman J.M., Hanson M.W., Sostman H.D., Schold S.C. (1991). Clinical application of PET for the evaluation of brain tumors. J Nucl Med.
2 Kaschten B., Stevenaert A., Sadzot B., Deprez M., Degueldre C., Del Fiore G., Luxen A., Reznik M. (1998). Preoperative evaluation of 54 gliomas by PET with fluorine-18-fluorodeoxyglucose and/or carbon-11-methionine. J Nucl Med.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
5 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
6 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
7 Palacin M., Estevez R., Bertran J., Zorzano A. (1998). Molecular biology of mammalian plasma membrane amino acid transporters. Physiol Rev.
8 Jarkas N., Voll R.J., Williams L., Camp V.M., Goodman M.M. (2010). (R,S)-anti-1-amino-2-[18F]fluorocyclopentyl-1-carboxylic acid: synthesis from racemic 2-benzyloxycyclopentanone and biological evaluation for brain tumor imaging with positron emission tomography. J Med Chem.
9 Savir-Baruch, B., D.M. Schuster, N. Jarkas, V.A. Master, P.T. Nieh, R.K. Halkar, J.A. Nye, M.M. Lewis, R.J. Crowe, R.J. Voll, V.M. Camp, L.M. Bellamy, D.L. Roberts, and M.M. Goodman, Pilot Evaluation of Anti-1-amino-2-[(18)F] fluorocyclopentane-1-carboxylic acid (anti-2-[(18)F] FACPC) PET-CT in Recurrent Prostate Carcinoma. Mol Imaging Biol, 2010
10 Oka S., Hattori R., Kurosaki F., Toyama M., Williams L.A., Yu W., Votaw J.R., Yoshida Y., Goodman M.M., Ito O. (2007). A preliminary study of anti-1-amino-3-18F-fluorocyclobutyl-1-carboxylic acid for the detection of prostate cancer. J Nucl Med.
11 Shoup T.M., Olson J., Hoffman J.M., Votaw J., Eshima D., Eshima L., Camp V.M., Stabin M., Votaw D., Goodman M.M. (1999). Synthesis and evaluation of [18F]1-amino-3-fluorocyclobutane-1-carboxylic acid to image brain tumors. J Nucl Med.